# ^89^Zr-Desferrioxamine p-isothiocyanatobenzyl-anti-hepatocyte growth factor nanobody 1E2 fused to albumin-binding nanobody Alb8

Chemical name: | ^89^Zr-Desferrioxamine p-isothiocyanatobenzyl-anti-hepatocyte growth factor nanobody 7D12 fused to albumin-binding nanobody Alb8
Abbreviated name: | ^89^Zr-Df-Bz-NCS-1E2-Alb8
Synonym: | ^89^Zr-1E2-Alb8
Agent category: | Antibody fragment, nanobody
Target: | Hepatocyte growth factor (HGF)
Target category: | Receptor
Method of detection: | Positron emission tomography
Source of signal: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/protein/AAA64297.1), nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NM_000601.4) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/gene/3082) for more information about HGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=1E2-Alb8)]

MET is a proto-oncogene protein, also known as c-Met or hepatocyte growth factor receptor (HGFR) (1). MET is a membrane receptor with tyrosine kinase activity that is essential for embryonic development and wound healing. MET is normally expressed by stem cells, progenitor cells, and cells of epithelial origin, whereas expression of hepatocyte growth factor (HGF), which is the only known ligand of MET, is restricted to cells of mesenchymal origin. Upon HGF stimulation, MET induces several biological responses that lead to invasive growth (2). Abnormal MET activation in cancer correlates with poor prognosis because deregulated MET triggers tumor growth, induces angiogenesis, and activates metastasis (3). MET and HGF are overexpressed in many types of human malignancies, including kidney, liver, stomach, breast, and brain cancers (2, 4, 5). Inhibition of MET function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (6). On the other hand, targeting HGF may also be beneficial to patients by blocking binding of HGF to MET.

Nanobodies are the smallest intact antigen-binding fragments (15 kDa) isolated from heavy-chained camelid antibodies, and they exhibit efficient and specific tumor targeting (7, 8). With circulating blood half-lives of <1 h, monospecific nanobodies may not efficiently block binding of growth factors to their receptors (9). In order to extend the half-life of the nanobody, Vosjan et al. (10) linked an anti-HGF 1E2 nanobody with an anti-albumin nanobody (Alb8) to form a bispecific molecule (1E2-Alb8). For use with positron emission tomography, 1E2-Alb8 was conjugated with the bifunctional chelate p-isothiocyanatobenzyl-desferrioxamine (Df-Bz-NCS) and labeled with ^89^Zr to form ^89^Zr-Df-Bz-NCS-1E2-Alb8 for imaging HGF expression in tumors.

### Related Resource Links:

- Chapters in MICAD (HGF (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HGF+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), c-Met (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=c-Met+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (HGF (http://www.ncbi.nlm.nih.gov/gene/3082), c-Met (http://www.ncbi.nlm.nih.gov/gene/4233))
- Articles in Online Mendelian Inheritance in Man (OMIM) (HGF (http://omim.org/entry/142409), c-Met (http://omim.org/entry/164860))
- Clinical trials (HGF (http://www.clinicaltrials.gov/ct2/results?term=hepatocyte+growth+factor), c-Met (http://www.clinicaltrials.gov/ct2/results?term=c-Met))
- Drug information in FDA (c-Met (http://google2.fda.gov/search?q=c-Met&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=12))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=1E2-Alb8+synthesis)]

Df-Bz-NCS-1E2-Alb8 was prepared by incubation of nanobody 1E2-Alb8 with Df-Bz-NCS in buffer (pH 9) for 30 min at 37°C (10). Df-Bz-NCS-1E2-Alb8 was purified with column chromatography. The number of Df-Bz-NCS groups per nanobody was not reported. For ^89^Zr-labeling, a solution of ^89^Zr and 1E2-Alb8 was incubated in HEPES buffer (pH 7.0) for 60 min at room temperature. The labeling yields were 75%–90%, with a radiochemical purity of >97%. The specific activity of ^89^Zr-Df-Bz-NCS-1E2-Alb8 was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=1E2-Alb8+in+vitro)]

Binding experiments with 1E2 and 6E10 with the use of a Biacore sensor chip immobilized with human HGF protein were performed with K_d_ values of 1.36 nM and 1.14 nM (10). 1E2 and 6E10 inhibited binding of HGF to MET with IC_50_ values of 1.8 nM and 3.0 nM, respectively. In cell-based assays, 1E2 and 6E10 inhibited HGF-induced MET phosphorylation in human epithelial cell carcinoma A549 cells and proliferation in human prostate carcinoma Bx-PC3 cells. The immunoreactivity of ^89^Zr-Df-Bz-NCS-1E2-Alb8 was 50% and similar to that of ^131^I-1E2-Alb8.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=1E2-Alb8+rodentia)]

Vosjan et al. (10) performed ex vivo biodistribution studies of 0.37 MBq (0.01 mCi) ^89^Zr-Df-Bz-NCS-1E2-Alb8 (1 nmol) in U87MG (human glioblastoma) tumor-bearing nude mice (n = 5/group) at 1, 2, 3, and 7 d after injection. Accumulation into U87MG tumors was 7.8 ± 1.1% injected dose/gram (ID/g), 8.9 ± 1.0% ID/g, 8.7 ± 1.5% ID/g, and 7.2 ± 1.6% ID/g at 1, 2, 3, and 7 d, respectively. Blood levels were 12.6 ± 0.7% ID/g, 7.2 ± 1.0% ID/g, 3.4 ± 0.3% ID/g, and 0.3 ± 0.1% ID/g at 1, 2, 3, and 7 d, respectively. Blood level at 1 h was 42% ID/g. Tumor accumulation levels were higher than the levels in normal organs, with the exception of the kidneys. The kidney accumulation levels were 50%–75% ID/g at 1–7 d. Another ^89^Zr-labeled nanobody, ^89^Zr-Df-Bz-NCS-6E10-Alb8, showed a similar pattern of ex vivo biodistribution in the same tumor model. No blocking studies and PET imaging were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=1E2-Alb8+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=1E2-Alb8+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=1E2-Alb8+human)]

No publication is currently available.

## NIH Support

5K08 CA102545-04

## References

1 Boccaccio C., Comoglio P.M. (2006). Invasive growth: a MET-driven genetic programme for cancer and stem cells. Nat Rev Cancer.
2 Di Renzo M.F., Olivero M., Giacomini A., Porte H., Chastre E., Mirossay L., Nordlinger B., Bretti S., Bottardi S., Giordano S., et al. (1995). Overexpression and amplification of the met/HGF receptor gene during the progression of colorectal cancer. Clin Cancer Res.
3 Lengyel E., Prechtel D., Resau J.H., Gauger K., Welk A., Lindemann K., Salanti G., Richter T., Knudsen B., Vande Woude G.F., Harbeck N. (2005). C-Met overexpression in node-positive breast cancer identifies patients with poor clinical outcome independent of Her2/neu. Int J Cancer.
4 Smith H.S., Stern R., Liu E., Benz C. (1991). Early and late events in the development of human breast cancer. Basic Life Sci.
5 Di Renzo M.F., Olivero M., Serini G., Orlandi F., Pilotti S., Belfiore A., Costantino A., Vigneri R., Angeli A., Pierotti M.A., et al. (1995). Overexpression of the c-MET/HGF receptor in human thyroid carcinomas derived from the follicular epithelium. J Endocrinol Invest.
6 Petrelli A., Circosta P., Granziero L., Mazzone M., Pisacane A., Fenoglio S., Comoglio P.M., Giordano S. (2006). Ab-induced ectodomain shedding mediates hepatocyte growth factor receptor down-regulation and hampers biological activity. Proc Natl Acad Sci U S A.
7 Desmyter A., Decanniere K., Muyldermans S., Wyns L. (2001). Antigen specificity and high affinity binding provided by one single loop of a camel single-domain antibody. J Biol Chem.
8 Muyldermans S., Cambillau C., Wyns L. (2001). Recognition of antigens by single-domain antibody fragments: the superfluous luxury of paired domains. Trends Biochem Sci.
9 Els Conrath K., Lauwereys M., Wyns L., Muyldermans S. (2001). Camel single-domain antibodies as modular building units in bispecific and bivalent antibody constructs. J Biol Chem.
10 Vosjan M.J., Vercammen J., Kolkman J.A., Stigter-van Walsum M., Revets H., van Dongen G.A. (2012). Nanobodies targeting the hepatocyte growth factor: potential new drugs for molecular cancer therapy. Mol Cancer Ther.